# N-[^11^C]Methyl-3-[[(dimethylamino)carbonyl]oxy]-2-(2’,2’-diphenylpropionoxymethyl)pyridinium

Chemical name: | N-[^11^C]methyl-3-[[(dimethylamino)carbonyl]oxy]-2-(2',2'-diphenylpropionoxymethyl)pyridinium
Abbreviated name: | [^11^C]MDDP
Synonym:
Agent Category: | Compound
Target: | Acetylcholinerase (AChE)
Target Category: | Binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20MDDP%5BAll%20Fields%5D)]

Acetylcholinerase (AChE) is an enzyme involved in terminating nerve impulses by hydrolyzing the neurotransmitter acetylcholine (ACh). It plays an important role in heart rate and cardiac contractions, for example, by decreasing the ACh levels associated with cardiac parasympathetic responses (1).

AChE, and more exactly the inhibition of its enzymatic function, also seems to play an important role in poisoning from organophosphorus (OP) agents (2). Current treatments consisting of a reversible covalent AChE inhibitor (pyridostigmine (3)), a receptor antagonist atropine (ATR), and a AChE reactivator (pralidoxime chloride) have shown good protection against OP intoxication in animals. Research efforts are being made to find drugs with multiple protective functions. For example, Leader et al. (4) synthesized and evaluated a group of pyridophen analogues, binary pyridogstigmine-aprophen prodrugs with differential inhibition of AChE, butyrylcholinesterase (BChE), and muscarinic receptors (5).

Most of the AChE heart tracers developed for cardiac neurotransmission using positron emission tomography (PET) have shown low selectivity of AChE over BChE, and non-specific binding in AChE enzyme overexpressed regions (6). [^11^C]Nedrophonium and [^11^C]Neostigmine, originally developed as potential PET heart imaging agents, have shown either high nonspecific binding or poor myocardial uptake and were therefore unsuitable for PET imaging of the heart vagal system.

[^11^C]pyridostigmine and its para- and ortho-analogs, as well as N-[^11^C]methyl-3-[[(dimethylamino)carbonyl]oxy]-2-(2',2'-diphenylpropionoxymethyl)pyridinium ([^11^C]MDDP), were synthesized by Wang et al. (7) as potential PET agents for imaging heart AChE in vivo. Leader et al. (4) showed that MDDP iodide selectively inhibited AChE more than BChE. However, the first rodent studies performed by Wang et al. (7) using PET- [^11^C]MDDP did show the presence of nonspecific binding (see the Rodents section for details).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29MDDP%20AND%20synthesis)]http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed

A multi-step synthesis procedure for [^11^C]MDDP was reported by Wang et al. (7) in 2005. The authors used a modified version of a method by Leader et al. (4) to obtain the precursor and reference standard. Briefly, the preparation of [^11^C]MDDP involved an acylation of the key intermediate 2-hydroxymethyl-3-dimethylaminocarbonyl-oxypyridine with 2,2-diphenylpropionyl chloride to produce the carbamyl-ester precursor 3-[[(dimethylamino)carbonyl]oxy]-2-(2',2'-diphenylpropionoxymethyl)pyridine in 51% yield.

The key intermediate used in this synthetic method was obtained in 31% yield from carbamylation of 3-hydroxy-2-hydroxymethylpyridine HCl with dimethylcarbamyl chloride; the acylation agent was produced in 96% yield from 2,2-diphenylpropionic acid with thionyl chloride in 96% yield.

The tertiary pyridine precursor was labeled with [^11^C]methyl triflate to provide the quaternary pyridinium tracer [^11^C]MDDP in 40–65% radiochemical yield (decay corrected at end of bombardment). The final product [^11^C]MDDP was eluted with an aqueous solution of 2% acetic acid (containing up to 8% ethanol to enhance recovery of some [^11^C-methyl]quaternary cations. The total synthesis time reported by Wang et al. (7) was 10–15 min. The chemical and radiochemical purities (determined by analytical HPLC) were >95% and >99% respectively. The specific radioactivity of the tracer [^11^C]MDDP was ~0.05 MBq/mol (1.0–1.5 Ci/μmol) at end of the synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29MDDP%20AND%20in%20vitro)]

In vitro studies performed by Leader et al. (4) showed that MDDP iodide preferentially inhibited AChE over BChE, and that the inhibition of both enzymes was at least as strong as that obtained with pyridogstigmine (8). The mean values of the affinity constant for the initial reaction obtained for AChE and BChE were 5.62 x 10^-6^ M and 3.14 x 10^-6^ M respectively. In comparison, for pyridostigmine, those values were 1.97 x 10^-5^ M (AChE) and 1.14 x 10^-4^ M (BChE).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29MDDP%20AND%20rodentia%5BMeSH%5D)]

Wang et al. (7) performed in vivo dynamic PET imaging studies using [^11^C]MDDP in 3 young adult female Sprague–Dawley rats for a 60min time period after intravenous injection of 7.4 MBq (0.2 mCi) of the tracer for each animal. Those studies showed a rapid heart uptake of the tracer, and a fast blood clearance in 10 to 20 min. The mean standard uptake value (SUV) for [^11^C]MDDP reported by the authors was 0.125 ± 0.034 (n = 3).

Competitive inhibition studies were then performed to assess the specificity of the tracer to heart tissue AChE. Animals were pretreated with an injection of the drug neostigmine, used as unlabeled AChE inhibitor. A partial blocking effect was observed. However, a t test comparing the mean SUVs with no blocking agent (0.125 ± 0.034) and with blocker neostigmine (0.128 ± 0.0066) led to a p value of 0.87, indicating no statistically significant difference between the two and therefore the presence of nonspecific binding. Wang et al. (7) also suggested the possibility of an insufficient blockade of cholinesterase binding sites, because 2 of 3 rats exhibited actual increases in [^11^C]MDDP retention after administration of neostigmine.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29MDDP%20AND%20%28dog%20OR%20pig%20OR%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29MDDP%20AND%20%28primates%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29MDDP%20AND%20human)]

No publication is currently available

## References

1 Gomez JL, Moral-Naranjo MT, Campoy FJ, Vidal CJ. (1999). Characterization of acetylcholinesterase and butyrylcholinesterase forms in normal and dystrophic Lama2dy mouse heart. J Neurosci Res.
2 Duysen EG, Li B, Xie W, Schopfer LM, Anderson RS, Broomfield CA, Lockridge O. (2001). Evidence for nonacetylcholinesterase targets of organophosphorus nerve agent: supersensitivity of acetylcholinesterase knockout mouse to VX lethality. J Pharmacol Exp Ther.
3 Dirnhuber P, French MC, Green DM, Leadbeater L, Stratton JA. (1979). The protection of primates against soman poisoning by pretreatment with pyridostigmine. J Pharm Pharmacol.
4 Leader H, Wolfe AD, Chiang PK, Gordon RK. (2002). Pyridophens: binary pyridostigmine-aprophen prodrugs with differential inhibition of acetylcholinesterase, butyrylcholinesterase, and muscarinic receptors. J Med Chem.
5 Leader H, Smejkal RM, Payne CS, Padilla FN, Doctor BP, Gordon RK, Chiang PK. (1989). Binary antidotes for organophosphate poisoning: aprophen analogues that are both antimuscarinics and carbamates. J Med Chem.
6 Ryu EK, Choe YS, Park EY, Paik JY, Kim YR, Lee KH, Choi Y, Kim SE, Kim BT. (2005). Synthesis and evaluation of 2-[18F]fluoro-CP-118,954 for the in vivo mapping of acetylcholinesterase. Nucl Med Biol.
7 Wang JQ, Miller MA, Mock BH, Lopshire JC, Groh WJ, Zipes DP, Hutchins GD, Zheng QH. (2005). Facile synthesis and PET imaging of a novel potential heart acetylcholinesterase tracer N-[11C]methyl-3-[[(dimethylamino)carbonyl]oxy]-2-(2',2'-diphenylpropionoxy methyl)pyridinium. Bioorg Med Chem Lett.
8 Main AR, Hastings FL. (1966). Carbamylation and binding constants for the inhibition of acetylcholinesterase by physostigmine (eserine). Science.